# Recombinant adenovirus with enhanced green fluorescent protein

Chemical name: | Recombinant adenovirus with enhanced green fluorescent protein
Abbreviated name: | Ad-E3-EGFP
Synonym:
Agent Category: | Adenovirus
Target: | Coxsackie-adenovirus receptor (CAR)
Target Category: | Receptor
Method of detection: | Fluorescence imaging, optical
Source of signal: | Green fluorescence protein
Activation: | Yes, viral replication required
Studies: | - In vitro; - Rodents | Click here for protein and nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=45827793) sequence of the Coxsackie-adenovirus receptor (CAR)

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=adenovirus+vectors&WebEnv=0TmycNTl_TB4i6LP0kdm3bA7ZrgmZj-Z7YLtg3N1Bn4PcaqefkML5zIHckST3Miq4I7sZi4GzkZWQ%407748428072881B60_0000SID&WebEnvRq=1)]

A variety of options, including surgery, radiation, chemotherapy, and biopharmaceuticals, or a combination of these therapies, have been developed and are commonly used for the treatment of cancer. However, these treatments often result in undesirable side effects for the patient and may not always be efficacious (1-3). As a result, the use of gene therapy as an alternative therapy for cancer has been developed and attempted by several investigators (4, 5). The adenovirus (Ad) is the most common vehicle used for the gene therapy of cancer, both as a vector and as an oncolytic agent (4, 5). The Ad is a non-enveloped DNA virus that binds to the Coxsackie-Ad receptor (CAR) on cells and has been studied for more than half a century. After binding to CAR, the virus interacts with the host cell integrins (which serve as secondary receptors) and is internalized by receptor-mediated endocytosis (6). A detailed description of Ad structure, gene composition, and biology is available elsewhere (7). Ad is one of the best-characterized viruses and, depending on the infecting serotype, is known to cause several different illnesses such as conjunctivitis, gastroenteritis, the common cold, and other respiratory ailments in humans (8, 9). There are ~50 serotypes of Ad, and among these Ad2 and Ad5 are the serotypes most commonly used for gene therapy. This is because Ad can be easily engineered to target a specific ailment such as cancer, can be made replication-deficient, does not integrate into the mammalian genome, can accommodate large transgenes, and can be modified to have a reduced immunological responses in mammals (10).

To make recombinant Ad suitable for use as a gene therapy vector, several strategies are used by investigators in the field (11). A common approach to generate an Ad vector is by substituting a viral gene(s) with the gene(s) of interest (11). For selective infection of cancerous tumors, conditionally replicating Ads (CRAds) have been generated that replicate only in the neoplastic cells and locally amplify the virus, which ultimately results in lysis of the host cell (thus the virus is oncolytic) (12). The lack of replication in normal tissue restricts the infection of CRAds to the cancerous cells, and the CRAds would replicate only until the cancerous cells are depleted. Other advantages of using CRAds for cancer therapy are discussed in detail by Kanerva and Hemminki (12). Although CRAds are being used in several clinical trials (http://clinicaltrials.gov/ct2/results?term=Adenovirus+cancer+gene+therapy&recr=&type=&cond=&intr=&spons=&id=&state1=&cntry1=&state2=&cntry2=&state3=&cntry3=&locn=&rcv_s=&rcv_e=) in the United States, still little is known regarding their replication, spreading ability, persistence, and interaction with the host system (13). According to Ono et al., this is probably because a non-invasive monitoring system was not available to investigate these CRAd parameters (13). Ono et al. envisioned that CRAds could probably be studied in an in vivo setting if the vector could be monitored with a fluorescent reporter gene (13).

This chapter details the development and in vitro and in vivo evaluation of a CRAd vector bearing the enhanced green fluorescent protein (EGFP) as the reporter gene (13).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=adenovirus+vector+synthesis&WebEnv=07lpcUPvQUm2EdXlvFfce7bqBf9Dp2EZ1dJejIkB0lyGGWcd08u2aDnWbLK__6IWQ-5_tHqz5cey3%407748428072881B60_0000SID&WebEnvRq=1)]

Synthesis of the recombinant CRAd described in this chapter was as detailed by Ono et al. (13). Using recombinant DNA and homologous recombination techniques, three vectors based on Ad5 were generated by deletion of the E3 region of the virus (for details of the Ad structure, see Rux and Burnett (7)). A commercially available plasmid was used as the source of the EGFP reporter gene inserted into each vector. Depending on the location of the EGFP gene in the recombinant virus genome, the vectors were designated as Ad-E3-EGFR F0, F1, and F2, respectively (13). The plasmids were then transfected into for initial vector production and subsequently propagated in A549 cells (http://www.biotech.ist.unige.it/cldb/cl207.html) (14). After propagation and harvesting, the recombinant vectors were purified twice by ultracentrifugation on a cesium chloride gradient and dialysis against phosphate-buffered saline containing magnesium, calcium, and glycerol. The titer of the viral particles and storage conditions for the final product were not reported by the investigators (13).

The EGFP signal could be detected with an excitation and emission bandpass filter combination with wavelengths of 490/10 and 535/30, respectively. The background autofluorescence was determined with a 560/10 and 605/55 combination filter. The background was subtracted from the fluorescence signal (13).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ad+E3+EFGP+in+vitro&WebEnv=0pNJCPKfn1pgj9WxTOnN0SXFW-i-1oqijaHZFN7pdOUpq9d5F6BFX3wto9NU0_FPqeRPPqztoQjBj%407748428072881B60_0000SID&WebEnvRq=1)]

The in vitro expression of EGFP for the three recombinant constructs was monitored in A549 cells that support Ad5 replication (13). For this study, chemically transformed BALB/c mouse hepatoma cells (BNL-1NG-A.2) were used as controls because they are not conducive to Ad5 replication. Depending on the viral dose used to infect the cells, all the replication-competent viruses were observed to show an increase in fluorescence over time with the A549 cells. In the same conditions and time period, no increase in fluorescence was observed with the BNL-1NG-A.2 cells. An increase in fluorescence from the transfected cells was observed only if the virus was in a replication-permissive environment. At higher multiplicities of infection (1 and 10 virus particles/cell), there was a sigmoid increase in fluorescence. The investigators suggested that the sigmoid curve was observed because, after the initial infection, there was a log phase of infection of the surrounding cells that was followed by exhaustion and death (oncolysis) of the replication-permissive cells. Among the various constructs, the F2 construct showed the highest EGFP expression as determined by fluorescence monitoring.

In the same study, the increase in fluorescence in the A549 cells over 5 days was shown to be dose-dependent and correlated with replication of the F2 viral DNA (13). During the same period, no change in fluorescence was observed with the BNL-1NG-A.2 cells. From these observations the investigators concluded that the EGFP reporter system could be used for in vitro monitoring of Ad replication.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ad+E3+EFGP+rodentia&WebEnv=0BGoy8fnqomqh5goPOrWfIkuS49Zxc81EnK_Yp8ZNHN9TeDsO6zOJ041RAi1Fqkgibx19wKfTADny%407748428072881B60_0000SID&WebEnvRq=1)]

A549 and BNL-1NG-A.2 cell tumors were established in athymic nude mice to evaluate the in vivo detection of Ad replication by fluorescence (13). A single injection of the F2 vector was administered directly into the tumors, and EGFP expression was detected and monitored with a non-invasive fluorescence optical imaging system. After imaging, the tumors were excised and the total Ad DNA copy number after replication was determined. A good correlation between the fluorescence and the DNA copy number was reported for the A549 cells. No fluorescence was observed with the BNL-1NG-A.2 tumors. Replication of the F2 vector in the A549 tumors was monitored over 19 days. During the initial week, an increase in fluorescence from the tumor was observed, followed by a gradual decline in the signal, indicating viral clearance. The investigators reported that the area of infected cells did not spread beyond the initial region of the fluorescence signal and suggested that this was probably because of the inability of the virus to cause oncolysis of the entire tumor (13). The investigators cautioned that, although the EGFP system could be used for non-invasive, in vivo monitoring of Ad replication, its reduced detectability in deep tissue could be a limitation for clinical use.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ad+E3+EFGP+Non+Primate+Mammals&WebEnv=0OTLCNxjuOGiJLE-NZkgrXsBDg8JuyEY9_yMTiQPMHLXwbg5SGsrm6iBL4d0w1zrXCjUAl_RgsTnH%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ad+E3+EFGP+Non+Human+Primates&WebEnv=0AD133TIUjpxQJEghEUbrYHl7oLDo362OUXUICpfLzyEQqinPdoF33NaWWT31IegqWcYPUt0FkFde%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ad+E3+EFGP+Human+Studies&WebEnv=0J8ZT6sh-ytLno-4IIisXnZQ1c18XZ-Oh9VU6efy7MXqw3n6xqfncD3Dho_OwOd9CQ4dqXX-TQ_Ng%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## NIH Support

Parts of the studies presented in this chapter were supported by NIH grants R01 DK063615, R01 CA094084 and 1P20CA101955.

## References

1 Bonner J.A., Ang K. (2007). More on severe cutaneous reaction with radiotherapy and cetuximab. N Engl J Med.
2 Budach W., Bolke E., Homey B. (2007). Severe cutaneous reaction during radiation therapy with concurrent cetuximab. N Engl J Med.
3. Hadji, P. and N. Bundred, Reducing the Risk of Cancer Treatment-Associated Bone Loss in Patients With Breast Cancer. Semin Oncol, 2007. 34S4: p. S4-S10.
4 Zhang X., Yang Z., Dong L., Papageorgiou A., McConkey D.J., Benedict W.F. (2007). Adenoviral-mediated interferon alpha overcomes resistance to the interferon protein in various cancer types and has marked bystander effects. Cancer Gene Ther.
5 Yang Z.R., Wang H.F., Zhao J., Peng Y.Y., Wang J., Guinn B.A., Huang L.Q. (2007). Recent developments in the use of adenoviruses and immunotoxins in cancer gene therapy. Cancer Gene Ther.
6 Wickham T.J., Mathias P., Cheresh D.A., Nemerow G.R. (1993). Integrins alpha v beta 3 and alpha v beta 5 promote adenovirus internalization but not virus attachment. Cell.
7 Rux J.J., Burnett R.M. (2004). Adenovirus structure. Hum Gene Ther.
8 Hayashi S., Hogg J.C. (2007). Adenovirus infections and lung disease. Curr Opin Pharmacol.
9 Jiang S.C. (2006). Human adenoviruses in water: occurrence and health implications: a critical review. Environ Sci Technol.
10 Tanaka T., Kuroki M., Hamada H., Kato K., Kinugasa T., Shibaguchi H., Zhao J., Kuroki M. (2007). Cancer-targeting gene therapy using tropism-modified adenovirus. Anticancer Res.
11 Douglas J.T. (2007). Adenoviral vectors for gene therapy. Mol Biotechnol.
12 Kanerva A., Hemminki A. (2005). Adenoviruses for treatment of cancer. Ann Med.
13 Ono H.A., Le L.P., Davydova J.G., Gavrikova T., Yamamoto M. (2005). Noninvasive visualization of adenovirus replication with a fluorescent reporter in the E3 region. Cancer Res.
14 Fallaux F.J., Kranenburg O., Cramer S.J., Houweling A., Van Ormondt H., Hoeben R.C., Van Der Eb A.J. (1996). Characterization of 911: a new helper cell line for the titration and propagation of early region 1-deleted adenoviral vectors. Hum Gene Ther.